# ^64^Cu-Labeled human serum albumin–conjugated Affibody Z_HER2:342_ that targets the human epidermal growth factor receptor 2 (HER2)

Chemical name: | ^64^Cu-Labeled human serum albumin–conjugated Affibody Z_HER2:342_ that targets the human epidermal growth factor receptor 2 (HER2)
Abbreviated name: | [^64^Cu]-DOTA-HSA-Z_HER2:342_
Synonym:
Agent Category: | Affibody (antibody)
Target: | Human epidermal growth factor receptor 2 (HER2)
Target Category: | Receptor
Method of detection: | Photon emission tomography (PET)
Source of signal / contrast: | ^64^Cu
Activation: | No
Studies: | - In; - vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=affibody&cmd=DetailsSearch)]

An Affibody molecule is a chain of 58 amino acids (~6.5 kDa) that contains a modified B domain of the staphylococcal protein A and can be obtained by chemical synthesis or produced in bacteria with the use of recombinant technology (1). Because of their small size and high chemical and thermal stability, these molecules are used as radiolabeled probes for the targeted detection and treatment of malignant tumors as discussed elsewhere (1-3). In this regard, the epidermal growth factor receptor 2 (HER2) is considered to be an important Affibody target because it is believed to promote development of the malignant phenotype, it plays a role in the development of resistance to anticancer drugs and radiation therapy, it is overexpressed in several different cancer tumor cells, and it often indicates a poor prognosis for the patient (4). Several radionuclide-labeled Affibodies or their derivatives, such as Z_HER2:342_, have been evaluated to detect tumors expressing HER2 in preclinical studies as discussed by Tolmachev (5). Although the labeled Affibodies generate high-contrast images of the tumors, a common limitation observed with these tracers is an elevated accumulation of radioactivity in the kidneys, which masks the detection of tumors in adjacent regions of these and other organs (6). In addition, there is also a concern that the high radiation dose(s) produced from radioactivity accumulated in the kidneys can damage these organs in some patients.

Human serum albumin (HSA) is a multifunctional nonimmunogenic circulatory protein (~65 kDa) that has good biocompatible and biodegradation characteristics, and recombinant HSA (rHSA) or its derivative can be used as an excipient to formulate biological drugs (http://www.drugdeliverytech.com/ME2/dirmod.asp?nm=Back+Issues&type=Publishing&mod=Publications::Article&mid=8F3A7027421841978F18BE895F87F791&tier=4&id=E939D76B10EB4A82A10CC28C2AD08B38) (7). In addition, because HSA has a long circulating half-life and is not eliminated through the kidneys, investigators have evaluated the use of rHSA-drug conjugates to improve the efficacy of drugs and to visualize tumors using a radiolabeled integrin receptor-binding peptide coupled to rHSA (6). On the basis of this information, Hoppmann et al. evaluated the ability of a ^64^Cu- or ^111^In-labeled 1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraaceticacid (DOTA)-HSA-Z_HER2:342_ Affibody conjugate to target and visualize xenograft SKOV3 cell (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=HTB-77&Template=cellBiology) tumors in mice with the use of positron emission tomography (PET; for the ^64^Cu-labeled Affibody) and single-photon emission tomography (SPECT; for the ^111^In-labeled Affibody), respectively. (6). This chapter describes the investigations performed with [^64^Cu]-DOTA-HSA-Z_HER2:342_. Studies performed with [^111^In]-DOTA-HSA-Z_HER2:342_ are presented in a separate chapter of MICAD (www.micad.nih.gov ) (8).

### Other Sources of Information

Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=affibody+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Other Epidermal growth factor receptor (EGFR) imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=EGFR+AND+micad%5Bbook%5D&doptcmdl=TOCView&log%24=booksrch&bname=micad)

EGFR (human) ligands (http://www.ncbi.nlm.nih.gov/pubmed?term=Human%20EGFR%20ligands&cmd=DetailsSearch) in PubMed.

Human EGFR in OMIM (http://www.ncbi.nlm.nih.gov/omim?term=Human%20EGFR) (Online Mendelian Inheritance in Man)

Information on EGFR (human) gene (http://www.ncbi.nlm.nih.gov/protein?Db=gene&Cmd=retrieve&dopt=full_report&list_uids=1956&log$=genesensor5&logdbfrom=protein)

Protein (http://www.ncbi.nlm.nih.gov/protein/NP_005219.2?ordinalpos=17&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum) and nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/NG_011529.1?ordinalpos=3&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum) information regarding EGFR

Anti-EGFR antibody clinical trials (http://clinicaltrials.gov/ct2/results?term=anti-EGFR+antibodies)

EGFR pathways (http://pid.nci.nih.gov/search/intermediate_landing.shtml?molecule=EGFR&Submit=Go) in Pathways Interaction Database

Production of rHSA in yeast (http://www.ncbi.nlm.nih.gov/pubmed?term=production%20of%20recombinant%20human%20serum%20albumin%20in%20yeast)

Protein and mRNA sequence (http://www.ncbi.nlm.nih.gov/nuccore/NM_000477.5) of human serum albumin

HSA clinical trials (http://clinicaltrials.gov/ct2/results?term=HSA)

Information regarding HSA on Food and Drug Administration web site (http://google2.fda.gov/search?q=human+serum+albumin&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-DOTA-HSA-ZHER2%3A342%20synthesis&cmd=DetailsSearch)]

The synthesis of DOTA-HSA-Z_HER2:342_ and its labeling with ^64^Cu have been described by Hoppmann et al. (6). Approximately 2 molecules of DOTA and 1–5 molecules of Z_HER2:342_ were reported to be conjugated to each HSA molecule as determined with matrix-assisted laser desorption/ionization-time of flight-mass spectroscopy. Denaturing polyacrylamide gel electrophoresis of DOTA-HSA-Z_HER2:342_ revealed a broad band on the gel because different numbers of the Affibody molecule were attached to each molecule of HSA. The radiochemical yield of the labeled Affibody was ~60%, with a specific activity of 12–14 MBq/nmol (0.32–0.37 mCi/nmol). The [^64^Cu]-DOTA-HSA-Z_HER2:342_ was formulated in phosphate-buffered saline (the purification buffer, pH not mentioned), and the stability of the labeled complex was not reported.

[^64^Cu]-DOTA-HSA was also produced for use as control for PET imaging (6). The radiochemical yield, purity, and specific activity of this radiolabeled compound were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-DOTA-HSA-ZHER2%3A342%20in%20vitro&cmd=DetailsSearch)]

The uptake of [^64^Cu]-DOTA-HSA-Z_HER2:342_ by SKOV3 cells was studied as described by Hoppmann et al. (6). Uptake of the radiochemical was observed to increase from 0.17 ± 0.05% (percent of added radioactivity) at 0.5 h to 1.58 ± 0.09% at 2 h. The pattern of [^64^Cu]-DOTA-HSA-Z_HER2:342_ uptake by the cells was similar to that observed with the ^111^In-labeled Affibody (6). Accumulation of the ^64^Cu-labeled Affibody in the cells was significantly inhibited (P < 0.05) in the presence of excess (2.12 μM) nonradioactive Affibody. This indicated that the ^64^Cu-labeled probe bound specifically to the epidermal growth factor receptor (EGFR) on the cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-DOTA-HSA-ZHER2%3A342%20rodentia&cmd=DetailsSearch)]

Mice (n = 3 animals per group) bearing SKOV3 cell tumors were injected with 5.2–7.4 MBq (140–200 μCi) [^64^Cu]-DOTA-HSA-Z_HER2:342_ through the tail vein, and PET images were acquired from the anesthetized animals (using 2% isoflurane) at 1, 4, 24, and 48 h postinjection (p.i.) as described by Hoppmann et al. (6). Tumor-bearing control animals received [^64^Cu]-DOTA-HSA and were imaged in the same way as the test animals. At 1 h p.i., the tumors were visible with a low tumor/background contrast, but the tumors were clearly visible at 4 h and 24 h p.i. and remained clear up to 48 h p.i. Quantification analysis of the images showed that the tumor uptake increased from 5.63 ± 2.07% injected dose per gram tissue (% ID/g) at 1 h to ~14% ID/g at 24 h p.i. and remained constant for up to 48 h p.i. The liver had an accumulation of 12.92 ± 2.4% ID/g at 24 h p.i., and the kidneys showed an uptake of 4.17 ± 1.01% ID/g at the same time point. The biodistribution of [^64^Cu]-DOTA-HSA in the animals was similar to that of the labeled Affibody, with the exception of a two- to three-fold lower uptake (P < 0.05) of labeled HSA in the tumors compared to that of [^64^Cu]-DOTA-HSA-Z_HER2:342_ at the various time points. These observations were similar to those obtained from the biodistribution and imaging studies performed with [^111^In]-DOTA-HSA-Z_HER2:342_ (6).

On the basis of the information obtained from this study, the investigators concluded that both [^64^Cu]-DOTA-HSA-Z_HER2:342_ and [^111^In]-DOTA-HSA-Z_HER2:342_ exhibited a high specificity for the detection of HER2-expressing tumors in rodents with the use of PET and SPECT imaging, respectively (6).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-DOTA-HSA-ZHER2%3A342%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-DOTA-HSA-ZHER2%3A342%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-DOTA-HSA-ZHER2%3A342%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

Work reported in this chapter was supported in part by National Cancer Institute (NCI) grant 5R01 CA119053 and NCI In Vivo Cellular Molecular Imaging Center (ICMIC) grant P50 CA114747.

## References

1 Feldwisch J., Tolmachev V., Lendel C., Herne N., Sjoberg A., Larsson B., Rosik D., Lindqvist E., Fant G., Hoiden-Guthenberg I., Galli J., Jonasson P., Abrahmsen L. (2010). Design of an optimized scaffold for affibody molecules. J Mol Biol.
2 Tolmachev V., Orlova A. (2010). Influence of labelling methods on biodistribution and imaging properties of radiolabelled peptides for visualisation of molecular therapeutic targets. Curr Med Chem.
3 Lofblom J., Feldwisch J., Tolmachev V., Carlsson J., Stahl S., Frejd F.Y. (2010). Affibody molecules: engineered proteins for therapeutic, diagnostic and biotechnological applications. FEBS Lett.
4 Capala J., Bouchelouche K. (2010). Molecular imaging of HER2-positive breast cancer: a step toward an individualized 'image and treat' strategy. Curr Opin Oncol.
5 Tolmachev V. (2008). Imaging of HER-2 overexpression in tumors for guiding therapy. Curr Pharm Des.
6 Hoppmann S., Miao Z., Liu S., Liu H., Ren G., Bao A., Cheng Z. (2011). Radiolabeled affibody-albumin bioconjugates for HER2-positive cancer targeting. Bioconjug Chem.
7 Chuang V.T., Otagiri M. (2007). Recombinant human serum albumin. Drugs Today (Barc).
8 Chopra, A., 111In-Labeled human serum albumin conjugated Affibody ZHER2:342 that targets the human epidermal growth factor receptor 2 (HER2). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.